# ^99m^Tc-Mercaptoacetyl-Glu-Glu-Glu-Affibody Z_HER2:342_

Chemical name: | ^99m^Tc-Mercaptoacetyl-Glu-Glu-Glu-Affibody Z_HER2:342_
Abbreviated name: | ^99m^Tc-MaEEE-Z_HER2:342_
Synonym:
Agent category: | Antibody fragment, Affibody
Target: | EGF HER2 receptor
Target category: | Receptor
Method of detection: | SPECT, gamma planar
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20)]

Epidermal growth factor (EGF) is a cytokine that comprises 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). Trastuzumab is approved for clinical use for anti-cancer therapies in both Europe and North America. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ eveloped for imaging human breast cancer (12-16). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed on the basis of the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A (17). Affibody molecules exhibit high binding affinity (K_d_) to HER2 with K_d_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. Mercaptoacetyl-Gly-Gly-Gly (MAG3) was used a chelating linker for coupling ^99m^Tc to Z_HER2:342_ Affibody (18). ^99m^Tc-MAG3-Z_HER2:342_ has been evaluated in nude mice bearing human colon adenocarcinoma tumors, resulting in high tumor/blood and tumor/muscle ratios. However, ^99m^Tc-MAG3-Z_HER2:342_ exhibited a high hepatobiliary clearance, which resulted in a high radioactivity in the intestines at 4 h after injection (19). Therefore, glutamic acid was used as the chelating linker to decrease the lipophilicity of Z_HER2:342_ Affibody to suppress hepatobiliary clearance (20). ^99m^Tc-Mercaptoacetyl-Glu-Glu-Glu-Affibody Z_HER2:342_ (^99m^Tc-MaEEE-Z_HER2:342_) was found to a have favorable biodistribution in nude mice bearing SKOV-3 tumors, resulting in a 3-fold lower hepatobiliary clearance than ^99m^Tc-MAG3-Z_HER2:342_.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20synthesis)]

Z_HER2:342_ Affibody was prepared by standard solid phase peptide synthesis. MaEEE-Z_HER2:342_ was prepared by addition of MaEEE to the N-terminal of the Z-Affibody (20). ^99m^Tc as pertechnetate was added to a solution of MaEEE-Z_HER2:342_ containing SnCl_2_. The mixture was incubated for 60 min at room temperature. The labeling efficiency of ^99m^Tc incorporation was 90 ± 2% with >98% purity. ^99m^Tc- MaEEE-Z_HER2:342_ was purified by size-exclusion chromatography. Specific activities of the preparations were not reported. ^99m^Tc-MaEEE-Z_HER2:342_ was found to be stable after incubation in murine blood plasma (>99%) at 37°C for 1 h or solution containing 300-fold excess cysteine (93 ± 3%) at 37°C for 2 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20in%20vitro)]

Tran et al. (20) performed binding experiments with MaEEE-Z_HER2:342_ with use of a Biacore sensor chip immobilized with extracellular domain of HER2 protein. The K_d_ values were 410 and 80 pM for MaEEE-Z_HER2:342_ and Z_HER2:342_, respectively. Hence, the binding affinity of the synthetic Affibody molecule MaEEE-Z_HER2:342_ was 4.1-fold lower than the parent Affibody molecule Z_HER2:342_. In vitro binding specificity tests showed that binding of ^99m^Tc-MaEEE-Z_HER2:342_ to SKOV-3 cells expressing HER2 was receptor-mediated because saturation of receptors by preincubation with non-labeled Z_HER2:342_ significantly decreased binding of ^99m^Tc-MaEEE-Z_HER2:342_. The antigen binding capacity of ^99m^Tc-MaEEE-Z_HER2:342_ was 67%. The cell-bound radioactivity remained constant at ~70% of the initially bound activity for up to 24 h when the cells were incubated with ^99m^Tc-MaEEE-Z_HER2:342_. In contrast, cells incubated with ^125^I-Z_HER2:342_ retained ~40% of the original cell-associated radioactivity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20rodentia)]

Tran et al. (20) performed biodistribution studies of 0.1 MBq (2.7 μCi) ^99m^Tc-MaEEE-Z_HER2:342_ in nude mice (n = 4) bearing SKOV-3 xenografts. ^99m^Tc-MaEEE-Z_HER2:342_ (0.14 nmol) was injected s.c. to each mouse. The initial tracer accumulation in the SKOV-3 tumors was 9.1% injected dose per gram (ID/g) at 1 h, 7.9% ID/g at 4 h and 6.1% ID/g 6 h after injection. The radioactivity level in tumors was higher than in other organs and tissues except the kidneys (>30% ID/g). Blood levels were ~2% ID/g at 1 h, and 0.15% ID/g at 6 h. The biodistribution was characterized by quick clearance of radioactivity from blood and all organs and tissues. The radioactivity of intestine content was <3% ID/g at 6 h. Tumor/blood ratios were 6, 38, and 43 at 1, 4, and 6 h after injection, respectively. Pre-administration of Z_HER2:342_ (83 nmol) decreased tumor accumulation from 7.9 ± 1.0 to 0.30 ± 0.07% ID/g (P <0.0001) at 4 h after injection. Biodistribution studies were also performed in normal NMRI mice (n = 4) without bearing any tumors at 4 h after injection. The results showed low accumulation in all organs and tissues except with 95% ID/g in the kidneys and ~3% ID in the intestines. Single-photon emission computed tomography (SPECT) analysis was performed in nude mice bearing the SKOV-3 tumors after i.v. injection of 3 MBq (81 μCi) ^99m^Tc-MaEEE. Tumor/muscle ratios were 8, 19, and 35 at 1, 2, and 5 h, respectively. No other organs were visualized except the kidneys. In mice pretreated with Z_HER2:342_, the tumors could not be clearly visualized with ^99m^Tc-MaEEE-Z_HER2:342_. Tumor/muscle ratio was 3.6.as measured at 5 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Engfeldt, T., A. Orlova, T. Tran, A. Bruskin, C. Widstrom, A.E. Karlstrom, and V. Tolmachev, Imaging of HER2-expressing tumours using a synthetic Affibody molecule containing the (99m)Tc-chelating mercaptoacetyl-glycyl-glycyl-glycyl (MAG3) sequence. Eur J Nucl Med Mol Imaging, 2006
19 Tran T., Engfeldt T., Orlova A., Widstrom C., Bruskin A., Tolmachev V., Karlstrom A.E. (2007). In vivo evaluation of cysteine-based chelators for attachment of 99mTc to tumor-targeting Affibody molecules. Bioconjug Chem.
20 Tran T., Engfeldt T., Orlova A., Sandstrom M., Feldwisch J., Abrahmsen L., Wennborg A., Tolmachev V., Karlstrom A.E. (2007). (99m)Tc-maEEE-Z(HER2:342), an Affibody molecule-based tracer for the detection of HER2 expression in malignant tumors. Bioconjug Chem.